# ^125^I-Vascular endothelial growth factor-121

Chemical name: | ^125^I-Vascular endothelial growth factor-121
Abbreviated name: | ^125^I-VEGF_121_
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor binding
Method of detection: | SPECT, planar gamma
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various number of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). ^123^I-VEGF_165_ has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). Yoshimoto et al. (9) compared biodistribution of ^125^I-VEGF_121_ and ^125^I-VEGF_165_ in an LS180 human colon tumor xenograft model to develop ^125^I-VEGF_121_ as an imaging agent to study tumor angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20synthesis)]

VEGF_121_ was labeled with sodium [^125^I]iodide by electrophilic radioiodination using the chloramine-T method (9). ^125^I-VEGF_121_ was purified by gel filtration. This method yielded a specific activity of 0.52–0.74 GBq/nmol (14–20 mCi/nmol). No yield or radiochemical purity values were reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20in%20vitro)]

^125^I-VEGF_121_ was stable in mouse serum for up to 4 h at 37°C, and no de-iodination was found (9). Li et al. (6) reported that ^123^I-VEGF_121_ (0.001 nM) induced proliferation of human umbilical vein endothelial cells to an extent similar to unlabeled VEGF_121_, and a high-affinity ^125^I-VEGF_121_ binding site (B_max1_ = 5840 ± 20 sites/cell, K_d_ = 80 ± 13 pM) was found on their cell surfaces.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20rodentia)]

Yoshimoto et al. (9) performed biodistribution studies of ^125^I-VEGF_121_ and ^125^I-VEGF_165_ in nude mice bearing an LS180 human colon tumor. The organs with the highest accumulation of ^125^I-VEGF_121_ (in percent of injected dose per gram (% ID/g)) were the uterus (13.76 ± 2.19% ID/g), lung (13.31 ± 2.05% ID/g), kidneys (11.46 ± 0.78% ID/g), tumor (9.12 ± 0.98% ID/g), stomach (8.81 ± 1.87% ID/g), and heart (8.39 ± 0.41% ID/g) at 2 h after injection. ^125^I-VEGF_165_ uptake in tumors was one-fold higher than that of ^125^I-VEGF_165_ (4.79 ± 1.08% ID/g at 2 h). ^125^I-VEGF_121_ exhibited a higher blood radioactivity than ^125^I-VEGF_165_ (32.03% versus 5.15% at 2 h). On the other hand, ^125^I-VEGF_165_ exhibited a higher accumulation in the stomach (32.79% versus 8.81% at 2 h). ^125^I-VEGF_121_ displayed higher tumor/non-tumor ratios in most normal organs than ^125^I-VEGF_165_ because ^125^I-VEGF_121_ was cleared more rapidly than ^125^I-VEGF_165_ from the normal organs. Autoradiographic and immunohistochemical analyses confirmed that the difference in ^125^I-VEGF_121_ tumor accumulation correlated with the degree of tumor vascularity. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I-VEGF%20AND%20human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Yoshimoto M., Kinuya S., Kawashima A., Nishii R., Yokoyama K., Kawai K. (2006). Radioiodinated VEGF to image tumor angiogenesis in a LS180 tumor xenograft model. Nucl Med Biol.